# [^111^In]Labeled-(NAc-dD-CHA-F-dS-dR-Y-L-W-S-βAla)_2_-K-K(DOTA)

Chemical name: | [^111^In]Labeled-(NAc-dD-CHA-F-dS-dR-Y-L-W-S-βAla)_2_-K-K(DOTA)
Abbreviated name: | [^111^In]Anti-uPAR peptide
Synonym:
Agent Category: | Compound
Target: | Urokinase-type plasminogen activator receptor (uPAR)
Target Category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[[underlined: PubMed]]

The urokinase-type plasminogen activator (uPA) is a serine protease that mediates its activity through a receptor (uPAR) and has an important role in several physiological processes such as matrix remodeling, inflammation, fibrinolysis, and cancer tumor angiogenesis, invasion, and metastasis (1). In addition, uPA activity is modulated by two specific inhibitors known as uPAI-1 and uPAI-2. The structure and functioning of uPA and its receptor is discussed in detail by Ploug (2). The uPA, uPAR, and the two inhibitors comprise the uPA system (uPAS), and any one or a combination of the uPAS components is known to be overexpressed in various malignant tumors, indicating a strong correlation of uPAS component overexpression to a poor prognostic outcome for the cancer patient (3). Therefore, investigators are interested in developing and evaluating agents that can be used non-invasively for the detection (e.g., by imaging techniques) and therapy (e.g., by radiotherapy with nuclide-containing uPAR ligands) of cancers that overexpress components of the uPAS. Li et al. recently reported the use of a linear, high-affinity uPAR antagonist, ^64^Cu-labeled peptide for the visualization of uPAR expression under preclinical conditions (4). In another study, Knor et al. evaluated and successfully used an α-emitting nuclide-conjugated peptide targeting the uPAR for the therapy of advanced ovarian cancer tumors in a mouse model (5). In a continued effort to develop and evaluate possible imaging agents for the visualization uPAR-expressing cancers, Liu et al. (6) synthesized and characterized a ^111^In-labeled (NAc-dD-CHA-F-dS-dR-Y-L-W-S-βAla)_2_-K-K(DOTA) peptide ([^111^In]anti-uPAR peptide; referred to as Test peptide from here on) under in vitro conditions and in mice bearing human breast cancer cell xenograft tumors.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B111In%5DAnti-uPAR%20peptide%20synthesis&cmd=DetailsSearch)]

Synthesis of the Test peptide has been discussed in detail by Liu et al. (6). The radiochemical yield, purity, and stability of the labeled compound were not reported. The specific activity of the Test peptide was reported to be 1.85–3.70 MBq/μg (50–100 μCi/μg).

A scrambled [^111^In]anti-uPAR peptide (referred to as Scrambled peptide from here on) was also synthesized for use as a negative control during the biodistribution studies. The radiochemical yield, purity, specific activity, and stability of the Scrambled peptide were not reported.

A ^125^I-labeled amino terminal fragment of uPA ([^125^I]ATF) that binds to the uPAR was also synthesized by the investigators for comparison with the Test peptide (6). However, the radiochemical yield, purity, specific activity, and stability of [^125^I]ATF were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Anti-uPAR%20peptide%20in%20vitro%20studies&cmd=DetailsSearch)]

To determine the binding affinity of the Test peptide, MDA-MB-231 human breast cancer cells were allowed to bind [^125^I]ATF in presence of increasing concentrations of the non-radioactive competitor peptides (6). Based on this study, the half maximal inhibitory concentration (IC_50_) of the Test peptide was reported to be 240 ± 125 nM, which was 300- to 600-fold higher than non-radioactive uPA or ATF (the IC_50_ values for uPA and ATF were 0.75 ± 0.01 and 0.44 ± 0.02 nM, respectively). This indicated that the anti-uPAR peptide had a lower affinity for uPAR than either uPA or ATF.

In another study, the investigators showed that cells obtained from the MDA-MB-231 xenograft tumors had a four- to five-fold lower uPAR occupancy compared to cells that had been stripped of the endogenous uPA using appropriate buffers (6). Using siRNA that inhibited the expression of uPA in MDA-MB-231 cells, the investigators showed that the specific binding of [^125^I]ATF to these cells was increased by ~4.4-fold (P < 0.01), and this increase in binding correlated well with the decrease observed in uPA mRNA and protein expression as determined with reverse transcriptase polymerase chain reaction and Western blot analysis, respectively (6). On the basis of these results, the investigators suggested that the high IC_50_ value observed for the anti-uPAR peptide (see above) could be due to receptor binding of the endogenous uPA. However, they did not explain why the IC_50_ values for uPA or ATF were lower than that of the Test peptide, given that the binding studies for all these peptides were performed under the same experimental conditions.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Anti-uPAR%20peptide%20rodentia&cmd=DetailsSearch)]

Biodistribution patterns of the Test peptide, the Scrambled peptide, and, for comparison, the [^125^I]ATF peptide were studied in severe combined immunodeficient mice bearing MDA-MB-231 xenograft tumors (6). The animals (n = 3 mice/time point per labeled compound) were injected with the respective radiochemicals via the tail vein and euthanized at 1, 4, and 24 h postinjection (p.i.) to determine the amount of radioactivity accumulated in the various organs, including the tumors. Both the Scrambled and the Test peptides had a rapid clearance from blood circulation, primarily through the urinary route. At 4 h p.i., the amount of radioactivity from the Test peptide that was accumulated in the blood, muscle, and the tumor was 0.06 ± 0.02% injected dose per gram tissue (% ID/g), 0.12 ± 0.06% ID/g, and 0.53 ± 0.11% ID/g, respectively. At the same time point, the amount of radioactivity in the blood, muscle, and the tumor from the Scrambled peptide was 0.15 ± 0.04% ID/g, 0.12 ± 0.02% ID/g, and 0.36 ± 0.05% ID/g, respectively. The accumulation of label in the tumor from the Test peptide was significantly (P < 0.05) higher than that from Scrambled peptide. No blocking studies were reported for the Test peptide. The accumulation of radioactivity from [^125^I]ATF in the tumor was not significantly higher than that of blood at all time points except at 24 h p.i. (0.26 ± 0.06% ID/g and 0.29 ± 0.06% ID/g in the blood and tumor, respectively). Also, co-injection of [^125^I]ATF with non-radioactive ATF was reported to reduce uptake of the label from this radiochemical significantly (P < 0.05) by 24 h p.i. in all organs, including the tumors (accumulation of radioactivity other time points was not reported).

The investigators report ongoing studies to determine the correlation between uPAR occupation by endogenous uPA and uptake of the radiotracer under in vivo conditions (6).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=anti%20upar%20peptide%20on%20primate%20mammals&cmd=DetailsSearch)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=anti%20upar%20peptide%20on%20human%20primates&cmd=DetailsSearch)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=anti%20upar%20peptide%20human%20studies&cmd=DetailsSearch)]

No references are currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## NIH Support

Some of the studies reported here were funded by National Cancer Institute Center grant I P50 CA103130-01.

## References

1 D'Alessio S., Blasi F. (2009). The urokinase receptor as an entertainer of signal transduction. Front Biosci.
2 Ploug M. (2003). Structure-function relationships in the interaction between the urokinase-type plasminogen activator and its receptor. Curr Pharm Des.
3 Ulisse S., Baldini E., Sorrenti S., D'Armiento M. (2009). The urokinase plasminogen activator system: a target for anti-cancer therapy. Curr Cancer Drug Targets.
4 Li Z.B., Niu G., Wang H., He L., Yang L., Ploug M., Chen X. (2008). Imaging of urokinase-type plasminogen activator receptor expression using a 64Cu-labeled linear peptide antagonist by microPET. Clin Cancer Res.
5 Knor S., Sato S., Huber T., Morgenstern A., Bruchertseifer F., Schmitt M., Kessler H., Senekowitsch-Schmidtke R., Magdolen V., Seidl C. (2008). Development and evaluation of peptidic ligands targeting tumour-associated urokinase plasminogen activator receptor (uPAR) for use in alpha-emitter therapy for disseminated ovarian cancer. Eur J Nucl Med Mol Imaging.
6 Liu D., Overbey D., Watkinson L., Giblin M.F. (2009). Synthesis and Characterization of an (111)In-Labeled Peptide for the in Vivo Localization of Human Cancers Expressing the Urokinase-Type Plasminogen Activator Receptor (uPAR). Bioconjug Chem.